# 1-([4-methoxy-^11^C]3,4-Dimethoxyphenethyl)-4-[3-(4-fluorophenyl)propyl]piperazine

Chemical name: | 1-([4-methoxy-^11^C]3,4-Dimethoxyphenethyl)-4-[3-(4-fluorophenyl)propyl]piperazine
Abbreviated name: | [^11^C]SA5845
Synonym:
Agent Category: | Compound
Target: | Sigma (σ) receptor
Target Category: | Receptor binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal/contrast: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SA5845)]

1-([4-methoxy-^11^C]-3,4-Dimethoxyphenethyl)-4-[3-(4-fluorophenyl)propyl]piperazine ([^11^C]SA5845) is a radioligand developed for positron emission tomography (PET) imaging of the sigma (σ) receptors. [^11^C]SA5845 is a potent σ receptor agonist labeled with ^11^C, a positron emitter with a physical half-life (t_½_) of 20.4 min (1).

σ receptors are functional, membrane-bound proteins distributed in the central nervous system (CNS) and peripheral organs such as the gastrointestinal tract and immune systems (2). The CNS σ receptors are unique binding sites related to higher brain functions (3). They are distinct from opiate and phencyclidine binding sites. There are at least two subtypes of σ receptors σ_1_ and σ_2_ receptors. The precise mechanism of the functional response of these receptors is not entirely known. These receptors appear to be involved in numerous pharmacological and physiologic functions, and they also modulate a number of central neurotransmitter systems, including noradrenergic, glutamatergic, and dopaminergic systems. phencyclidine and derivatives, cocaine and derivatives, some neuroleptics, atypical antipsychotic agents, and other chemically unrelated compounds can bind to the σ receptor sites. Studies have shown that these receptors may play a role in pathogenesis of psychiatric disorders (4, 5). These receptors are also expressed on a number of human and murine tumors (6).

The σ_1_ receptor subtypes have a molecular weight of ≈25 kDa, and through the process of cloning they have shown a 30% sequence homology with the yeast C89-C7 sterol isomerase (2, 7, 8) The σ_2_ receptor subtypes have a molecular weight of ≈21.5 kDa and have not been cloned. The σ_1_ receptors are thought to be involved in certain neuropsychiatric disorders, and the σ_2_ receptors are also implicated in malignant neoplastic diseases. Because of these effects, σ receptor ligands may be useful for detection and treatment in neurology and oncology. Matsuno et al. (9) developed a potent σ_1_ agonist, 1-(3,4-dimethoxyphenethyl)-4-(3-phenylpropyl)-piperazine dihydrochloride (SA4503), which is highly selective for σ_1_ receptors versus σ_2_ receptors. Small modifications in the SA4503 structure appear to have profound effects on the σ_1_/σ_2_ receptor affinity and selectivity (10). Fujimura et al. (11) prepared its fluorinated analog, SA5845, and reported that this compound had a high affinity for σ receptors. Kawamura et al. (12, 13) radiolabeled SA5845 with ^11^C and evaluated its potential for PET studies of σ receptors in CNS and tumors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SA5845%20AND%20synthesis)]

Kawamura et al. (12) reported the synthesis of the precursor 4-O-demethyl SA5845 for radiosynthesis of [^11^C]SA5845. 4-O-demethyl SA5845 was prepared from 4-fluorocinnamic acid by an eight-step synthesis. In the radiosynthesis of [^11^C]SA5845, [^11^C]methyl iodide was prepared and trapped in 0.2 ml of N,N-dimethylformamide containing 4-O-demethyl SA5845 and 1−2 mg of sodium hydride. The mixture was heated at 120ºC for 1 min, and then 1.3 ml of 0.1 M hydrochloric acid/[50 mM acetic acid/ammonium acetate, 1/1](35/65) was added. The reaction mixture was purified by high-performance liquid chromatography (HPLC). [^11^C]SA5845 was obtained with a radiochemical yield of 24 ± 4.2% (n = 6) in a synthesis time of 20 min. The radiochemical purity was >99%, and the specific activity was 135 TBq/mmol (3,645 Ci/mmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SA5845%20AND%20in%20vitro)]

Kawamura et al. (12) studied the in vitro properties of SA5845. The lipophilicity indicator logP_7.4_ (n-octanol/phosphate buffer at 37ºC) was determined to be 2.6. In comparison, the logP_7.4_ of SA4503 was 2.5. Using guinea pig brain membranes, the in vitro binding affinity (IC_50_) values of SA5845 to σ_1_ and σ_2_ receptors were 33 nM and 9.5 nM, respectively. Thus, the σ_2_/σ_1_ selectivity ratio was 0.29.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SA5845%20AND%20rodentia)]

Ex vivo brain autoradiography was carried out in rats with a [^11^C]SA5845 dose of 98−180 MBq/2.1−7.6 nmol (2.64−4.86 mCi/2.7−7.6 nmol) (12). The radioligand showed a higher density in the vestibular nucleus, temporal cortex, cingulated cortex, inferior colliculus, thalamus, and frontal cortex. A lower level of density was found in the hippocampus and cerebellum. The study indicated that this regional brain distribution pattern was very similar to other σ ligands.

In a mouse biodistribution study, each mouse (n = 4-5) received a dose of 1.0-2.0 MBq/8.2-34 pmol (27−54 μCi/8.2−34 pmol) (12). At 5 min after injection, the radioactivity levels measured as percentage of injected dose per g (% ID/g) were 2.87 ± 0.39 (brain), 0.85 ± 0.11 (blood), 21.4 ± 3.82 (lung), 7.18 ± 1.22 (liver), 12.5 ± 1.87 (kidney), and 1.63 ± 0.22 (muscle). At 60 min, these levels changed to 3.79 ± 0.32 (brain), 0.28 ± 0.08 (blood), 6.83 ± 1.65 (lung), 13.5 ± 1.49 (liver), 7.05 ± 0.78 (kidney), and 0.81 ± 0.13 (muscle). The brain radioactivity level increased for 60 min, whereas the radioactivity levels in the lung and kidney rapidly decreased. The brain radioactivity level was significantly decreased (60%) by co-injection of unlabeled SA5845 (2000 nmol/kg). Loading of haloperidol, a non-subtype-selective σ receptor ligand, loading also significantly decreased the brain radioactivity level.

Each mouse received 4.5−19 MBq/0.13−2.0 nmol (122−513 μCi/0.13−2.0 nmol) in a metabolite study using HPLC analysis (12). The percentages of unchanged [^11^C]SA5845 in the brain and plasma 30 min after injection were 98 ± 0.2 (n = 3) and 69 ± 3.1, respectively. [^11^C]SA5845 appeared to be very stable in the brain.

Kawamura et al. (13) performed tissue distribution studies of [^11^C]SA5845 in rats bearing the AH109A hepatoma.. The AH109A hepatoma was found to express a moderate density of both σ_2_ and σ_1_ receptors. Each mouse (n = 5) received 11 MBq/0.3 nmol (0.3 mCi/0,3 nmol) of [^11^C]SA5845. The tumor radioactivity levels (% ID/g) were 0.24 ± 0.08, 0.26 ± 0.06, 0.37 ± 0.04, and 0.49 ± 0.05 at 5, 15, 30, and 60 min after injection, respectively. PET images (14 MBq/1.28 nmol (0.38 mCi/1.28 nmol)) visualized the AH109A hepatoma on the rat thigh. The brain radioactivity levels were 0.94 ± 0.12, 0.88 ± 0.29, 0.89 ± 0.04, and 0.98 ± 0.07 at 5, 15, 30, and 60 min after injection, respectively. Co-injection with 1 mg/kg haloperidol significantly decreased the radioactivity levels at 30 min in the brain, kidney, and muscle. The radioactivity levels in the tumor and blood were significantly increased. The 30−min tumor/blood ratio decreased from 9.7 without haloperidol to 5.6 with haloperidol whereas the 30−min tumor/muscle ratio increased from 1.3 without haloperidol to 3.5 with haloperidol. At 30 min after injection, HPLC analysis showed that 95.4 ± 1.9% and 75.1 ± 7.9% of [^11^C]SA5845 remained unchanged in the tumor and plasma, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SA5845%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

Kawamura et al. (13) used PET imaging to study [^11^C]SA5845 in rabbits bearing the VX-2 carcinoma. In the VX-2 carcinoma the density of σ_2_ receptors was >10-fold than that of σ_1_ receptors. Each rabbit received 86 MBq/0.78 nmol (2.3 mCi/0.78 nmol) of [^11^C]SA5845. PET images clearly visualized VX-2 carcinoma on the rabbit thigh. The radioactivity level of the tumor increased for the first 10 min and then remained constant for 60 min. Pretreatment with 1 mg/kg haloperidol decreased the initial radioactivity level of [^11^C]SA5845 by 26% which then decreased further with time. Treatment with 1 mg/kg unlabeled SA5845 decreased the tumor radioactivity level by 53%. The authors concluded that [^11^C]SA5845 might be a potential radioligand for PET imaging of σ receptor−rich tumors.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SA5845%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=SA5845%20AND%20human)]

No publication is currently available.

## References

1 Kawamura K., Ishiwata K., Tajima H., Ishii S., Matsuno K., Homma Y., Senda M. (2000). In vivo evaluation of [(11)C]SA4503 as a PET ligand for mapping CNS sigma(1) receptors. Nucl Med Biol.
2 Lever J.R., Gustafson J.L., Xu R., Allmon R.L., Lever S.Z. (2006). Sigma1 and sigma2 receptor binding affinity and selectivity of SA4503 and fluoroethyl SA4503. Synapse.
3 Skuza G., Wedzony K. (2004). Behavioral pharmacology of sigma-ligands. Pharmacopsychiatry.
4 Skuza G. (2003). Potential antidepressant activity of sigma ligands. Pol J Pharmacol.
5 Ishiguro H., Ohtsuki T., Toru M., Itokawa M., Aoki J., Shibuya H., Kurumaji A., Okubo Y., Iwawaki A., Ota K., Shimizu H., Hamaguchi H., Arinami T. (1998). Association between polymorphisms in the type 1 sigma receptor gene and schizophrenia. Neurosci Lett.
6 Vilner B.J., John C.S., Bowen W.D. (1995). Sigma-1 and sigma-2 receptors are expressed in a wide variety of human and rodent tumor cell lines. Cancer Res.
7 Mach R.H., Gage H.D., Buchheimer N., Huang Y., Kuhner R., Wu L., Morton T.E., Ehrenkaufer R.L. (2005). N-[18F]4'-fluorobenzylpiperidin-4yl-(2-fluorophenyl) acetamide ([18F]FBFPA): a potential fluorine-18 labeled PET radiotracer for imaging sigma-1 receptors in the CNS. Synapse.
8 Hanner M., Moebius F.F., Flandorfer A., Knaus H.G., Striessnig J., Kempner E., Glossmann H. (1996). Purification, molecular cloning, and expression of the mammalian sigma1-binding site. Proc Natl Acad Sci U S A.
9 Matsuno K., Nakazawa M., Okamoto K., Kawashima Y., Mita S. (1996). Binding properties of SA4503, a novel and selective sigma 1 receptor agonist. Eur J Pharmacol.
10 Elsinga P.H., Kawamura K., Kobayashi T., Tsukada H., Senda M., Vaalburg W., Ishiwata K. (2002). Synthesis and evaluation of [18F]fluoroethyl SA4503 as a PET ligand for the sigma receptor. Synapse.
11 Fujimura K., Matsumoto J., Niwa M., Kobayashi T., Kawashima Y., In Y., Ishida T. (1997). Synthesis, structure and quantitative structure-activity relationships of sigma receptor ligands, 1-[2-(3,4-dimethoxyphenyl)ethyl]-4-(3-phenylpropyl) piperazines. Bioorg Med Chem.
12 Kawamura K., Elsinga P.H., Kobayashi T., Ishii S., Wang W.F., Matsuno K., Vaalburg W., Ishiwata K. (2003). Synthesis and evaluation of 11C- and 18F-labeled 1-[2-(4-alkoxy-3-methoxyphenyl)ethyl]-4-(3-phenylpropyl)piperazines as sigma receptor ligands for positron emission tomography studies. Nucl Med Biol.
13 Kawamura K., Kubota K., Kobayashi T., Elsinga P.H., Ono M., Maeda M., Ishiwata K. (2005). Evaluation of [11C]SA5845 and [11C]SA4503 for imaging of sigma receptors in tumors by animal PET. Ann Nucl Med.